# Cy5.5-Gly-Pro-Leu-Gly-Val-Arg-Gly-Cys-Ferritin-black hole quencher-3 nanocages

Chemical name: | Cy5.5-Gly-Pro-Leu-Gly-Val-Arg-Gly-Cys-Ferritin-black hole quencher-3 nanocages
Abbreviated name: | C/B-Fn nanocages
Synonym:
Agent category: | Peptide
Target: | Matrix metalloproteinases (MMPs)
Target category: | Enzyme
Method of detection: | Optical, near-infrared (NIR) fluorescence
Source of signal: | Cy5.5
Activation: | Yes
Studies: | - In vitro; - Rodents | No structure is currently available in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=RGD4C)]

Optical fluorescence imaging is increasingly used to monitor biological functions of specific targets in small animals (1-3). However, the intrinsic fluorescence of biomolecules poses a problem when fluorophores that absorb visible light (350–700 nm) are used. Near-infrared (NIR) fluorescence (700–1,000 nm) detection avoids the background fluorescence interference of natural biomolecules, providing a high contrast between target and background tissues. NIR fluorophores have a wider dynamic range and minimal background as a result of reduced scattering compared with visible fluorescence detection. They also have high sensitivity, resulting from low fluorescence background, and high extinction coefficients, which provide high quantum yields. The NIR region is also compatible with solid-state optical components, such as diode lasers and silicon detectors. NIR fluorescence (NIRF) imaging is becoming a noninvasive alternative to radionuclide imaging in small animals (4, 5).

Extracellular matrix (ECM) adhesion molecules consist of a complex network of fibronectins, collagens, chondroitins, laminins, glycoproteins, heparin sulfate, tenascins, and proteoglycans that surround connective tissue cells, and they are mainly secreted by fibroblasts, chondroblasts, and osteoblasts (6). Cell substrate adhesion molecules are considered essential regulators of cell migration, differentiation, and tissue integrity and remodeling. These molecules play a role in inflammation and atherogenesis, but they also participate in the process of invasion and metastasis of malignant cells in the host tissue (7). ECM provides a matrix environment for permeation of tumor cells through the basal lamina and underlying interstitial stroma of the connective tissue. Overexpression of matrix metalloproteinases (MMPs) and other proteases by tumor cells allows intravasation of tumor cells into the circulatory system after degrading the basement membrane and ECM (8).

Several families of MMPs are involved in atherogenesis, myocardial infarction, angiogenesis, and tumor invasion and metastases (9-12). MMP expression in normal cells, such as trophoblasts, osteoclasts, neutrophils, and macrophages, is highly regulated. Elevated levels of MMPs have been found in tumors associated with a poor prognosis for cancer patients (13). A peptide, Gly-Pro-Leu-Gly-Val-Arg-Gly-Cys-NH_2_, was found to be a MMP substrate and is cleaved between Leu and Gly residues. Lee et al. (14) used this sequence with a Cy5.5 NIR dye molecule to attach to AuNPs to form fluorescence-quenched Cy5.5-Gly-Pro-Leu-Gly-Val-Arg-Gly-Cys-AuNPs (Cy5.5-MMP-AuNPs). The Cy5.5 molecules are in close proximity, resulting in fluorescence quenching because of efficient fluorescence resonance energy transfer to Au. The NIR fluorescence signal will increase when the Leu-Gly bond is cleaved by MMPs, releasing fragments containing Cy5.5. Cy5.5 is a NIR fluorescent dye with absorbance maximum at 675 nm and emission maximum at 694 nm with a high extinction coefficient of 250,000 M−^1^cm−^1^. Cy5.5-MMP-AuNPs are being developed for NIR fluorescence imaging of MMP expression in tumors, atherosclerosis, myocardial infarction, and other diseases.

Ferritin is composed of 24 subunits of heavy and light chains that self-assemble to form a cage-like nanoparticle (nanocage) at physiological pH (7.4) with internal and external diameters of 8 nm and 12 nm (15, 16), respectively. The outer surface of ferritin can be chemically or genetically modified with ligands, and the cavity of ferritin can capture metal ions with high affinity (17). Lin et al. (18) chemically coupled Cy5.5-Gly-Pro-Leu-Gly-Val-Arg-Gly-Cys and black hole quencher-3 (BHQ-3) onto heavy chain ferritin to form C-Fn and B-Fn, respectively. Hybridization of C-Fn and B-Fn (1:1) resulted in the formation of C/B-Fn nanocages. The Cy5.5 molecules are in close proximity to BHQ-3, resulting in fluorescence quenching. NIR fluorescence signal will increase when the Leu-Gly bond is cleaved by MMPs, releasing fragments containing Cy5.5. C/B-Fn nanocages have been developed for NIRF imaging of tumor vasculature to study in vivo biodistribution of the tracer in tumor-bearing mice.

### Related Resource Links:

- Chapters in MICAD (MMP (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=books&Cmd=DetailsSearch&Term=MMP+AND+micad%5Bbook%5D))
- Gene information in NCBI (MMP13 (http://www.ncbi.nlm.nih.gov/gene/4322), ferritin heavy chain (http://www.ncbi.nlm.nih.gov/gene/2495), ferritin light chain (http://www.ncbi.nlm.nih.gov/gene/2512))
- Articles in Online Mendelian Inheritance in Man (OMIM) (MMP13 (http://www.ncbi.nlm.nih.gov/omim/600108))
- Clinical trials (MMP (http://www.clinicaltrials.gov/ct2/results?term=matrix+metalloproteinases+))
- Drug information in FDA (MMP (http://google2.fda.gov/search?q=matrix+metalloproteinases+&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=10&y=10))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=RGD4C+synthesis)]

Recombinant Fn subunits were purified from transfected Escherichia coli cell lysates (18). Fn nanocages were conjugated with a bifunctional compound, N-succinimidyl-4-maleimidobutyrate, and then with Cy5.5-Gly-Pro-Leu-Gly-Val-Arg-Gly-Cys to form C-Fn nanocages. BHQ-3 was conjugated to a different set of Fn nanocages to form B-Fn nanocages. There was one dye/quencher per Fn subunit. To prepare C/B-Fn nanocages, C-Fn and B-Fn nanocages (1:1 ratio) were broken down to subunits by adjusting pH to 2. The pH was then adjusted back to pH 7.4 with 1 M NaOH, and the mixture was incubated for 30 min to form C/B-Fn nanocages. C/B-Fn nanocages were isolated with column chromatography. The diameter of C/B-Fn nanocages was determined to be ~10 nm with dynamic light scattering analysis at pH 7.4

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=RGD4C+in%20vitro)]

C-Fn (430 nM) and B-Fn nanocages (430 nM) were decomposed in acidic buffer (pH 2) into C-Fn and B-Fn subunits (18). There was a maximal NIRF intensity (excitation at 675 nm, emission at 690 nm). The pH was then adjusted back to pH 7.4 with 1 M NaOH. There was a marked decrease in NIRF signal as the subunits reassembled into C/B-Fn nanocages. Addition of MMP13 (100 nM) restored the NIRF as MMP13 cleaved the Leu-Gly bond, releasing fragments containing Cy5.5. Incubation of C/B-Fn nanocages (C/B = 1:1) with 0.1–5 nM MMP13 for 30 min at 37°C showed that the activation of NIRF intensity depended on MMP concentration.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=RGD4C+rodentia)]

Lin et al. (18) performed whole-body NIRF imaging in nude mice (n = 3) bearing human UM-SCC-22B (head and neck squamous cell carcinoma) tumors at 30, 60, 90, 120, and 180 min after intratumoral injection of 0.02 mg C/B-Fn nanocages. There was an instant response upon injection, and the NIRF signal developed steadily at the tumor area in the first 120 min. Intratumoral pretreatment with MMP inhibitor III (a broad spectrum MMP inhibitor, 30 min before C/B-Fn nanocages) showed decreased NIRF intensities in the tumor area at all the time points studied.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=RGD4C+and%20%28dog%20or%20pig%20or%20sheep%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=RGD4C+and%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=RGD4C+human)]

No publication is currently available.

## NIH Support

Intramural Research Program

## References

1 Achilefu S. (2004). Lighting up tumors with receptor-specific optical molecular probes. Technol Cancer Res Treat.
2 Ntziachristos V., Bremer C., Weissleder R. (2003). Fluorescence imaging with near-infrared light: new technological advances that enable in vivo molecular imaging. Eur Radiol.
3 Becker A., et al. (2001). Receptor-targeted optical imaging of tumors with near-infrared fluorescent ligands. Nat Biotechnol.
4 Gurfinkel M., et al. (2003). Near-infrared fluorescence optical imaging and tomography. Dis Markers.
5 Tung C.H. (2004). Fluorescent peptide probes for in vivo diagnostic imaging. Biopolymers.
6 Bosman F.T., Stamenkovic I. (2003). Functional structure and composition of the extracellular matrix. J Pathol.
7 Jiang W.G., Puntis M.C., Hallett M.B. (1994). Molecular and cellular basis of cancer invasion and metastasis: implications for treatment. Br J Surg.
8 Albelda S.M. (1993). Role of integrins and other cell adhesion molecules in tumor progression and metastasis. Lab Invest.
9 Keppler D., et al. (1996). Tumor progression and angiogenesis: cathepsin B & Co. Biochem Cell Biol.
10 Liu J., et al. (2004). Lysosomal cysteine proteases in atherosclerosis. Arterioscler Thromb Vasc Biol.
11 Berchem G., et al. (2002). Cathepsin-D affects multiple tumor progression steps in vivo: proliferation, angiogenesis and apoptosis. Oncogene.
12 Brix, K., et al., Cysteine cathepsins: Cellular roadmap to different functions. Biochimie, 2007
13 Deryugina E.I., Quigley J.P. (2006). Matrix metalloproteinases and tumor metastasis. Cancer Metastasis Rev.
14 Lee S., et al. (2008). A near-infrared-fluorescence-quenched gold-nanoparticle imaging probe for in vivo drug screening and protease activity determination. Angew Chem Int Ed Engl.
15 Maham A., et al. (2009). Protein-based nanomedicine platforms for drug delivery. Small.
16 Uchida M., et al. (2010). The ferritin superfamily: Supramolecular templates for materials synthesis. Biochim Biophys Acta.
17 Uchida M., et al. (2006). Targeting of cancer cells with ferrimagnetic ferritin cage nanoparticles. J Am Chem Soc.
18 Lin X., et al. (2011). Hybrid ferritin nanoparticles as activatable probes for tumor imaging. Angew Chem Int Ed Engl.